# Microbubbles with a disteroylphosphatidylcholine, disteroylphosphatidylethanolamine-polyethyleneglycol (PEG) 2000-pyridyldithio propionate-PEG 40 stearate shell conjugated to cyclic arginine-glycine-aspartic acid-d-tyrosine-lysine (cRGD) pentapeptide

Chemical name: | Microbubbles with a disteroylphosphatidylcholine, disteroylphosphatidylethanolamine-polyethylene glycol (PEG) 2000-pyridyldithio propionate-PEG 40 stearate shell conjugated to cyclic arginine-glycine-aspartic acid-D-tyrosine-lysine (cRGD) pentapeptide
Abbreviated name: | cRGD-MB
Synonym:
Agent Category: | Peptide
Target: | α_v_β_3_ integrin receptor
Target Category: | Receptors
Method of detection: | Ultrasound imaging
Source of signal / contrast: | MIcrobubbles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ultrasound%20microbubbles%20targeting%20integrins&cmd=DetailsSearch)]

Ultrasonography (ultrasound) is a technique for the noninvasive imaging of tumors because it is easy to use, is relatively inexpensive compared to other imaging modalities, does not use radionuclides or x-rays, and produces real-time images (1, 2). Imaging with this modality may involve the use of ultrasound contrast agents (UCA) based on microbubbles (MB), which are made up of a thin, biodegradable, lipid or polymeric shell filled with various types of gases, such as perfluorocarbon, sulphur hexafluoride, decafluorobutane, etc (3, 4). Because of their size and structural features, the MB cannot permeate the extracellular spaces, so they stay in the vascular circulation until the core gas diffuses into the blood and the remaining shell is metabolized (2). When exposed to a narrow range of ultrasound frequencies (3–5 MHz), the gas in the MB resonates with the sound; this in turn causes the MB to oscillate, which generates a signature acoustic echo (signal) that can be captured with a transducer and converted into a signal to generate an image. The application of ultrasound in medicine has been discussed in detail elsewhere (5).

Investigators have recently become interested in the use of targeted UCA for the detection of malignant tumors because these agents can be directed to bind to specific molecules that are overexpressed on the surface of cells in cancerous tissues (4). An additional advantage of using targeted UCA with ultrasonography is that malignant lesions can be visualized noninvasively, whereas tumors can be overlooked during a visual ex vivo examination of tissues obtained after a biopsy. Tumors with a malignant phenotype are known to show elevated angiogenic activity (development of new vasculature from old blood vessels), and endothelial cells in the vasculature of these lesions show increased expression of certain cell surface molecules such as α_v_β_3_ integrins (6). The α_v_β_3_ integrins are heterodimeric transmembrane cell adhesion molecules that are recognized biomarkers of angiogenesis, tumor progression, and metastasis, and they are overexpressed in a variety of cancers (6). Integrins are targeted by a variety of antagonist drugs that can prevent tumor progression (6), and they are also used with imaging agents, including UCA, for the noninvasive visualization of tumors (4).

Most targeted MB have traditionally been prepared with either avidin or biotin as the coupling agents, and these MB could not be used in the clinical setting because of their potential immunogenicity (4). In an effort to alleviate this problem, lipid-based (liposomal) MB with pyridyldithio propionate (PDP) on the surface were prepared and conjugated to a cyclic arginine-glycine-aspartic acid motif (cRGD) containing pentapeptide (such peptides are known to have a high affinity for α_v_β_3_ integrins (7)) to generate cRGD-MB. The cRGD-MB were evaluated for use in imaging the cancerous lesion vasculature in mice bearing tumors generated with bEnd.3 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2299&Template=cellBiology) (mouse endothelial cells that express α_v_β_3_ integrins as confirmed with flow cytometry) (4).

### Other Sources of Information

MICAD (http://www.ncbi.nlm.nih.gov/books/?term=integrin++AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters related to integrins

Homo sapiens integrin alpha V, transcript variant 1, protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_002210.3) sequences

Integrin alpha V in Gene database (http://www.ncbi.nlm.nih.gov/gene/3685), Gene ID: 3685

Homo sapiens integrin beta 3, protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_000212.2) sequences

Integrin beta 3 in Gene database (http://www.ncbi.nlm.nih.gov/gene/374209), Gene ID: 374209

Clinical trials (http://clinicaltrials.gov/ct2/results?term=integrins) involving integrins

Integrins in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim?term=integrin%20) (OMIM) database

Integrin signaling pathways in Pathway Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100123&pathway_name=integrin%20signaling%20pathway&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cRGD%20Microbubble%20synthesis&cmd=DetailsSearch)]

MB with a disteroylphosphatidylcholine, disteroylphosphatidylethanolamine-polyethylene glycol (PEG) 2000-PDP-PEG 40 stearate shell (PDP-MB) were prepared as described by Anderson et al. (4). In some preparations, ~2% moles of Dil, a commercially available fluorescent membrane probe, was included in the reaction mixture for the detection of MB during ex vivo fluorescence microscopy. The PDP-MB were conjugated with the cRGD pentapeptide as detailed elsewhere (4). For some studies, MB containing a fluorescein isothiocyanate (FITC) derivative of cRGD (FITC-cRGD-MB) were prepared as described above. Control MB containing a non-binding scrambled cRAD pentapeptide (arginine-alanine-aspartic acid) were also prepared as described above.

The mean diameters of the control MB and the targeted MB were 2.75 ± 0.02 μm and 2.71 ± 0.01 μm, respectively, and <2% of the MB had a diameter >8.0 μm. The concentrations of the control MB and the targeted MB in the final preparations were reported to be 133 ± 8.0 × 10^7^/mL and 148 ± 1.1 × 10^7^/mL, respectively. Fluorescence spectroscopy of the FITC-cRGD-MB preparation revealed that 8.2 ± 1.6 × 10^6^ cRGD peptides were conjugated to each targeted MB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cRGD%20Microbubble%20in%20vitro&cmd=DetailsSearch)]

Parallel plate flow chamber assays showed that the adhesion of cRGD-MB to recombinant α_v_β_3_ integrin substrates was significantly higher (37.5 ± 9.2 MB/field of view (FOV); P < 0.01) than adhesion to a casein surface (0.7 ± 0.5 MB/FOV) or to an α_v_β_3_ integrin surface blocked with an anti-α_v_β_3_ integrin antibody (3.9 ± 1.5 MB/FOV) (4). The cRAD-MB exhibited minimal binding to any one of these surfaces.

In another study in which bEnd.3 cells were exposed to cRGD-MB alone, the MB showed >5-fold higher binding than cRAD-MB, PDP-MB, and cells treated with antibodies blocking either the α_v_ or the β_3_ integrin subunit (4). This indicated that the cRGD-MB bound specifically to the α_v_β_3_ integrin receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cRGD-MB%20rodentia&cmd=DetailsSearch)]

Ultrasound imaging was performed on Friend leukemia virus B–sensitive inbred mice bearing metastatic breast cancer Met-1 cell tumors as described by Anderson et al. (4). The animals were administered cRGD-MB and either cRAD-MB (n = 6 mice) or PDP-MB (n = 4 mice) via bolus through the tail vein, and images were acquired in a random order from the animals in each group. There was a 5-min delay between each imaging session, and a high-power ultrasound pulse was introduced to destroy MB from the previous study. Ultrasound imaging was performed with a protocol that could distinguish between the contrast echoes obtained from the target-bound and the free circulating MB as detailed elsewhere (4). Application of a high-powered ultrasound destruction sequence at 7 min after injection was shown to minimize the signal obtained from any circulating MB; this time point was selected for comparison of images obtained from the different MB treatment groups. Images obtained from mice treated with cRGD-MB clearly showed the tumor size and border and were easily distinguished from baseline images obtained before treatment with the UCA. The accumulation of targeted MB in the tumor vasculature of these animals was confirmed ex vivo with confocal microscopy using Dil-cRGD-MB as described by Anderson et al. (4).

In another study, the binding specificity of cRGD-MB was investigated in mice bearing Met-1 cell tumors after the animals (n = 6) were treated with a monoclonal antibody (mAb) that blocked the α_v_β_3_ integrins (4). The mice were administered cRGD-MB to establish baseline adhesion of the UCA in the tumors, and the animals were injected with ~700 pmol anti-α_v_β_3_ integrin mAb at 5 min after injection of cRGD-MB. At 30 min after the mAb treatment, the animals were again injected with cRGD-MB, and ultrasound imaging was performed to assess binding of the MB to the target. The tumor image intensity obtained from the mAb-treated animals was reported to be reduced by 3.2-fold compared to the intensity observed before the mAb treatment (baseline image). This indicated that the cRGD-MB bound specifically to the α_v_β_3_ integrins.

Administration of the soluble cRGD pentapeptide (~1 μmol) to the mice (n = 10) 30 min prior to the cRGD-MB injection did not block binding of the UCA to the tumor vasculature (4). The investigators have proposed several reasons for this observation, including rapid clearance of the peptide from the intravascular spaces due to its low molecular weight (~500 kDa), which may have reduced the local concentration of cRGD such that it was insufficient to block the α_v_β_3_ integrin receptors (4).

On the basis of these results, the investigators concluded that the cRGD-MB had good binding specificity for the α_v_β_3_ integrins and was a suitable UCA to visualize tumor angiogenesis (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cRGD-MB%20Other%20Non-Primate%20Mammals%20Studies&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cRGD-MB%20Non-Human%20Primates%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cRGD-MB%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported by National Institutes of Health grants IR43CA137913, 2R44EB007857, R01CA134659, R01CA112356, and R01CA103828.

## References

1 Eisenbrey J.R., Forsberg F. (2010). Contrast-enhanced ultrasound for molecular imaging of angiogenesis. Eur J Nucl Med Mol Imaging.
2 Wilson S.R., Burns P.N. (2010). Microbubble-enhanced US in body imaging: what role?. Radiology.
3 Deshpande N., Needles A., Willmann J.K. (2010). Molecular ultrasound imaging: current status and future directions. Clin Radiol.
4 Anderson C.R., Hu X., Zhang H., Tlaxca J., Decleves A.E., Houghtaling R., Sharma K., Lawrence M., Ferrara K.W., Rychak J.J. (2011). Ultrasound molecular imaging of tumor angiogenesis with an integrin targeted microbubble contrast agent. Invest Radiol.
5 Moore C.L., Copel J.A. (2011). Point-of-care ultrasonography. N Engl J Med.
6 Desgrosellier J.S., Cheresh D.A. (2010). Integrins in cancer: biological implications and therapeutic opportunities. Nat Rev Cancer.
7 Liu S. (2009). Radiolabeled cyclic RGD peptides as integrin alpha(v)beta(3)-targeted radiotracers: maximizing binding affinity via bivalency. Bioconjug Chem.